# 125I-Labeled trivalent, bispecific monoclonal antibody construct TF10 that targets mucin-1 and is reactive against a histamine-succinyl-glycine hapten IMP-288

Chemical name: | ^125^I-Labeled trivalent, bispecific monoclonal antibody construct TF10 that targets mucin-1 and is reactive against a histamine-succinyl-glycine hapten IMP-288
Abbreviated name: | [^125^I]-TP10
Synonym:
Agent Category: | Antibody
Target: | Mucin-1
Target Category: | Antigen
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging
Source of signal / contrast: | 125I
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Pretargeting%20antibodies&cmd=DetailsSearch)]

Most individuals suffering from pancreatic adenocarcinoma (PAC) do not survive for more than 1 year after diagnosis, and <1% of these patients live beyond 5 years (1). Although surgical resection of the cancer is a possible intervention for this disease, only 10%–25% of the patients are considered suitable for this treatment because, by the time that the neoplasm is detected, the malignancy has metastasized to other organs and the tumor load in the patient is too high to warrant surgery (2). Patients with nonresectable PAC are treated either with gemcitabine (http://www.cancer.gov/cancertopics/druginfo/gemcitabinehydrochloride) or radiotherapy or a combination of the two; however, these treatments are not curative because they only prolong survival and improve the quality of life of the patient (2). Early detection of this invasive cancer would facilitate proper staging of the disease so that a suitable treatment regimen can be initiated to possibly improve patient prognosis (3).

In this regard, the monoclonal antibody (mAb) PAM4, which specifically targets mucin 1 (MUC1), a glycoprotein that is overexpressed only in PAC tumors, was developed, radiolabeled with ^131^I or ^111^In, and shown with scintigraphy to detect neoplastic tumors in patients with pancreatic malignancies (4). However, intact radiolabeled antibodies (5) are known to have incomplete tumor penetration due to their large size (~150 kDa), and they are of limited utility to visualize cancerous lesions with different imaging modalities because they have a long blood circulating half-life and usually generate a low signal/noise (S/N) ratio (5). To amplify the signal obtained from an imaging agent so that it can be used to detect malignant tumors noninvasively, investigators have developed and evaluated a variety of strategies in preclinical studies with animals. One such strategy involves the pretargeting of cancer lesions with a suitable mAb (or its derivative), allowing some time for the pretargeting Ab to bind to the cancerous tissue and clear from blood circulation; the animals subsequently are injected with an appropriate radiolabeled small molecular weight ligand that binds to the pretargeting mAb or its derivative. This technique has been shown to generate higher S/N ratios during imaging compared to ratios obtained with a directly labeled mAb alone (6-8). Use of the pretargeting technique with multivalent (i.e., containing more than one antigen binding site), multispecific (i.e., can bind more than a single type of antigen) Abs for the imaging and therapy of cancer has been discussed in detail elsewhere (9, 10).

Cardillo et al. developed bsPAM4 (or bsmAb), a divalent, bispecific F(ab’)_2_ mAb, by cross-linking a PAM4 Fab’ fragment to a murine anti–In-diethylenetriamine pentaacetic acid (In-DTPA) mAb Fab’ fragment and used the unlabeled bsPAM4 to pretarget human CaPan-1 cell xenograft PAC tumors in nude mice (4). The animals were then exposed to a radiolabeled peptide hapten that bound to the In-DTPA binding mAb Fab’; imaging showed that this technique generated higher S/N ratios compared to the directly labeled bsmAb alone. From this study, the investigators concluded that the peptide was suitable for use with scintigraphy to target and visualize human xenograft PAC tumors in nude mice (4). In an effort to further improve the S/N ratio that can be obtained with the pretargeting technique, Gold et al. generated a recombinant trivalent (i.e., three binding sites) bsmAb, designated TF10, and evaluated its use with scintigraphy for the visualization of xenograft PAC tumors in mice (1). The TF10 bsmAb is divalent for binding to MUC1 and monovalent for binding to a histamine-succinyl-glycine (HSG) motif containing hapten (DOTA-D-Tyr-D-Lys(HSG)-D-Glu-D-Lys(HSG)-NH_2_ (IMP-288, HSG hapten)), and was generated by linking two PAM4 Fab fragments to an anti-HSG hapten mAb Fab fragment as described elsewhere (1). The biodistribution of ^125^I-labeled TF10 ([^125^I]-TF10) was studied in mice bearing PAC tumors and is discussed in this chapter. The biodistribution of ^111^In-labeled IMP-288 ([^111^In]-IMP-288) and the visualization of PAC tumors in mice with this labeled hapten is discussed in a separate chapter of MICAD (www.micad.nih.gov) (11).

### Related Resource Links

Peptide haptens [PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=peptide%20haptens&cmd=DetailsSearch)]

Clinical trials (http://clinicaltrials.gov/ct2/results?term=bispecific+antibody) with bispecific antibodies

Application of multivalent antibodies [PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=application%20of%20multivalent%20antibodies&cmd=DetailsSearch)]

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=125I-TF10%20synthesis&cmd=DetailsSearch)]

The recombinant synthesis of TF10 with the “dock-and-lock” method and the ^125^I labeling of the bsmAb with the Iodogen procedure have been described by Gold et al. (1). The specific activity of [^125^I]-TF10 was reported to be 14.8 kBq/pmol (0.4 μCi/pmol). Although the purity of the radiolabeled bsmAb was not reported, it was ascertained with size-exclusion high-performance liquid chromatography, and the amount of free isotope in the preparation was determined with instant thin-layer chromatography. The radiochemical yield of the final product was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=125-TF10&cmd=DetailsSearch)]

The binding of TF10 to the MUC1 antigen was investigated with an ELISA assay and compared to the binding of the PAM4 and PAM4 F(ab’)_2_ mAbs (1). These mAbs exhibited similar binding curves, and the half-maximal binding values of the mAbs were estimated to be 1.42 ± 0.10, 1.31 ± 0.12, and 1.83 ± 0.16 nmol/L, respectively (P = 0.05 for all). In comparison, bsPAM4 had a half-maximal binding of 30.61 ± 2.05 nmol/L (P = 0.0379), indicating that TF10 bound the antigen in a divalent manner (1). The immunoreactivity of ^125^I-TF10 to the MUC1 antigen was reported to be 87%, with 9% remaining unbound and 3% free ^125^I, as determined with low-pressure size-exclusion chromatography.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=125-TF10%20rodentia&cmd=DetailsSearch)]

The biodistribution of [^125^I]-TF10 was investigated in athymic nude mice bearing subcutaneous human xenograft pancreatic adenocarcinoma CaPan-1 cell tumors (1). The animals (n = 5 mice /group) were injected with the radioiodinated bsmAb (10 μCi (40 μg)) and euthanized at predetermined time points to determine the amount of radioactivity that accumulated in the various organs, including the tumors. Data obtained from this study were presented as a percent of injected dose per gram tissue (% ID/g).

Rapid clearance of radioactivity from the blood was observed with [^125^I]-TF10, decreasing from 21.03 ± 1.93% ID/g at 1 h postinjection (p.i.) to 0.13 ± 0.2% ID/g at 16 h p.i. and 0.03 ± 0.01% ID/g at 72 h p.i. Accumulation of the label in the lungs, liver, kidneys, and spleen ranged from ~6% ID/g (lungs) to ~12% ID/g (spleen) at 1 h p.i. and decreased to ~0.10% ID/g (kidneys) and ~0.17% ID/g (lungs and spleen) at 16 h p.i. Tumor uptake of the tracer peaked at 6 h p.i. (7.17 ± 1.10% ID/g) and decreased to 3.47 ± 0.66% ID/g at 16 h p.i. and 1.34 ± 0.24% ID/g at 72 h p.i. The biodistribution of [^125^I]-TF10 in the major organs of normal athymic nude mice (without tumors) was reported to be the same as mentioned above (data not presented), indicating that the tumors had no effect on the tissue-binding characteristics of the radioiodinated trivalent bsmAb (1). No blocking studies were reported.

From this study, the investigators concluded that TF10 was suitable to pretarget human xenograft tumors in mice (1).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=125-TF10%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=125-TF10%20Non-Human%20Primates&cmd=DetailsSearch)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=125-TF10%20Human%20Studies&cmd=DetailsSearch)]

No publication is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## NIH Support

Supported by National Cancer Institute, National Institutes of Health, grants CA096924 and CA115755.

## References

1 Gold D.V., et al. (2008). A novel bispecific, trivalent antibody construct for targeting pancreatic carcinoma. Cancer Res.
2 Gold D.V., et al. (2001). Localization of pancreatic cancer with radiolabeled monoclonal antibody PAM4. Crit Rev Oncol Hematol.
3 Gold D.V., et al. (2010). Detection of early-stage pancreatic adenocarcinoma. Cancer Epidemiol Biomarkers Prev.
4 Cardillo T.M., et al. (2004). Improved targeting of pancreatic cancer: experimental studies of a new bispecific antibody, pretargeting enhancement system for immunoscintigraphy. Clin Cancer Res.
5 Ahlgren S., et al. (2010). Targeting of HER2-expressing tumors using 111In-ABY-025, a second-generation affibody molecule with a fundamentally reengineered scaffold. J Nucl Med.
6 Forster G.J., et al. (2006). Pretargeted radioimmunotherapy with a single-chain antibody/streptavidin construct and radiolabeled DOTA-biotin: strategies for reduction of the renal dose. J Nucl Med.
7 Liu G., et al. (2010). Tumor pretargeting in mice using MORF conjugated CC49 antibody and radiolabeled complimentary cMORF effector. Q J Nucl Med Mol Imaging.
8 Uppal J.K., et al. (2011). Biological evaluation of avidin-based tumor pretargeting with DOTA-Triazole-Biotin constructed via versatile Cu(I) catalyzed click chemistry. J Drug Target.
9 Goldenberg D.M., Sharkey R.M. (2010). Radioactive antibodies: a historical review of selective targeting and treatment of cancer. Hosp Pract (Minneap).
10 Sharkey R.M., Goldenberg D.M. (2011). Cancer radioimmunotherapy. Immunotherapy.
11 Chopra, A., 111In-Labeled 1,4,7,10-Tetraazacyclododecane-N,N',N'',N'''-tetraaceticacid (DOTA)-d-Tyr-d-Lys(HSG)-d-Glu-d-Lys(HSG)-NH2 (IMP-288). Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.